# Cy7-Tyr-D-Glu-Cys-Hyp-Tyr(3-Cl)-Gly-Leu-Cys-Tyr-Ile-Gln-NH_2_

Chemical name: | Cy7-Tyr-D-Glu-Cys-Hyp-Tyr(3-Cl)-Gly-Leu-Cys-Tyr-Ile-Gln-NH_2_
Abbreviated name: | Cy7-FTP11
Synonym:
Agent category: | Peptide
Target: | Fibrin
Target category: | Acceptor
Method of detection: | Near-infrared (NIR) fluorescence imaging, optical
Source of signal/contrast: | Cy7
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FTP11)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-4). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–650 nm) are used. Near-infrared (NIR) fluorescence (650–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Extracellular matrix adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (6). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (7). A meshwork of clotted plasma protein was present in the tumor stroma but not in normal tissues, providing a functional matrix for angiogenesis, cell migration, and tumor cell invasion (8). There are high levels of collagens, fibronectin, and fibrin in the tumor connective tissues.

Thrombosis plays a major role in many cardiovascular diseases such as myocardial infarction, pulmonary embolism, deep venous thrombosis, and cerebral venous thrombosis (9). Thrombosis occurs by an activation process of thrombin (F2 coagulation factor II), which then converts fibrinogen into fibrin. Thrombin initiates the cross-linking of the polymerized fibrin via the activation of a transglutamase enzyme called coagulation factor XIII (FXIIIa indicates activated factor XIII) (10). Atherosclerotic lesions often contain microthrombi and fibrin on their surface. Fibrin is associated with a variety of malignant tumors. Fibrin is essential for stroma formation in the tumor with deposition of fibrin, which leads to tumor angiogenesis and metastasis. Hara et al. (11) prepared Cy7-Tyr-D-Glu-Cys-Hyp-Tyr(3-Cl)-Gly-Leu-Cys-Tyr-Ile-Gln-NH_2_ (Cy7-FTP11) for use with NIR fluorescence imaging of fibrin in thrombi in mice using high-resolution intravital fluorescence microscopy and fluorescence molecular tomography.

### Related Resource Links:

- Chapters in MICAD (fibrin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=fibrin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (fibrinogen (http://www.ncbi.nlm.nih.gov/gene/2243), fibronectin (http://www.ncbi.nlm.nih.gov/gene/2335))
- Articles in Online Mendelian Inheritance in Man (OMIM) (fibrinogen (http://www.ncbi.nlm.nih.gov/omim/134820), fibronectin (http://omim.org/entry/135600))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FTP11+synthesis)]

FTP11 was synthesized with solid-phase peptide synthesis (11). Cy7 was conjugated to the N-terminal amino group of FTP11 with addition of Cy7-succinimidyl ester. Cy7-FTP11 was isolated with high-performance liquid chromatography and cyclized by oxidation in dimethyl sulfoxide with >98% purity. Cy7-FTP11 exhibited an expected molecular mass of 2.62 kDa using matrix-assisted laser desorption/ionization mass spectrometry.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FTP11+in+vitro)]

In vitro fluorescence reflective imaging studies showed that Cy7-FTP11 exhibited significantly higher (P < 0.0001) target/background ratios (TBR) than free Cy7 to fibrin in human plasma clots, with TBRs of 6.30 ± 0.34 and 1.20 ± 0.03 (11), respectively. Excess unlabeled FTP11 (100-fold) inhibited the TBR of Cy7-FTP11 to 2.50 ± 0.34 (P < 0.05).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FTP11+rodentia)]

Intravital fluorescence microscopy imaging studies were performed in mice (n = 5/group) with the femoral vein exposed and treated with 7.5% FeCl_3_ solution to induce acute (2 h) and sub-acute (72 h) thrombosis (11). Cy7 or Cy7-FTP11 (150 nmol/kg) was injected via retro-orbital administration. NIR fluorescence signal (TBRs) increased in both acute (3.5 ± 0.3) and sub-acute (2.7 ± 05) thrombi at 60 min after injection of Cy7-FTP11, whereas no increase was observed with Cy7 (0.46 ± 0.08). Blocking studies were performed in mice (n = 4/group) with acute thrombosis after pretreatment with 100-fold excess unlabeled FTP11 (1,500 nmol/kg) 30 min before Cy7-FTP11 (15 nmol/kg) injection. Thrombus TBR at 60 min decreased from 1.60 ± 0.11 to 0.99 ± 0.04 (P < 0.01). Histostaining of the veins confirmed the localization of NIR fluorescence signals in the thrombi. Cy7-FTP11 exhibited a blood half-life of 2.82 min (n = 5).

Noninvasive fluorescence molecular tomography imaging studies were performed in mice with the left jugular vein treated with 7.5% FeCl_3_ solution to induce sub-acute thrombosis (11). The contralateral right jugular vein was sham-operated. FMT signals from jugular veins were co-registered with anatomic computed tomography images. The TBR of the left jugular vein thrombi (3.5 ± 0.7) was 1.3-fold higher than that of the contralateral right jugular vein (1.5 ± 0.3) (P < 0.05). Ex vivo NIR fluorescence signals were 3.9 ± 0.4 and 2.4 ± 0.4 (P < 0.05) for the left and right jugular veins, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FTP11+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FTP11+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FTP11+human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Leung K., Chopra A., Shan L., Eckelman W.C., Menkens A.E. (2012). Essential parameters to consider for the characterization of optical imaging probes. Nanomedicine (Lond).
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
7 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
8 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
9 Corti R., Fuster V. (2003). New understanding, diagnosis, and prognosis of atherothrombosis and the role of imaging. Am J Cardiol.
10 Lee K.N., Lee C.S., Tae W.C., Jackson K.W., Christiansen V.J., McKee P.A. (2001). Crosslinking of alpha 2-antiplasmin to fibrin. Ann N Y Acad Sci.
11 Hara T., Bhayana B., Thompson B., Kessinger C.W., Khatri A., McCarthy J.R., Weissleder R., Lin C.P., Tearney G.J., Jaffer F.A. (2012). Molecular imaging of fibrin deposition in deep vein thrombosis using fibrin-targeted near-infrared fluorescence. JACC Cardiovasc Imaging.